# [^131^I]N-(6-amino-2,2,4-trimethylhexyl)-2-[(5-iodo(3-pyridyl))carbonylamino]-3-(2-napthyl)propanamide

Chemical name: | [^131^I]N-(6-amino-2,2,4-trimethylhexyl)-2-[(5-iodo(3-pyridyl))carbonylamino]-3-(2-napthyl)propanamide
Abbreviated name: | [^131^I]IPC-β-AL3; [^131^I]IPC-AL3; ([underlined: 7])
Synonym:
Agent Category: | Ligand
Target: | Somatostatin receptor 1 (SSTR1)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IPC+beta+AL3)]

An autoimmune process and other environmental factors that destroy pancreatic β cells in the pancreatic islet cells are known to promote the development of insulin-dependent diabetes mellitus (type 1 diabetes) in individuals genetically predisposed to the disease (1). As a consequence of the β cell destruction, the net mass of these cells in the islet cells is reduced and, due to reduced insulin production, maintenance of blood glucose to a proper physiological level is impaired. The most common type of diabetes, type 2, is primarily caused by insulin resistance as a result of low insulin secretion by the β cells. Type 2 diabetes can often be corrected with exercise, diet control, and, if necessary, medication (2). On diagnosis of diabetes, knowledge of the β cell mass (BCM) or volume is an important factor to devise a successful treatment for the condition (3). Changes in the BCM during the onset of diabetes is poorly understood, and only an indirect method that measures the amount of simulated insulin secretion by the pancreas is used to quantify the BCM in humans (4). However, the β cells appear to have a reserved capacity to produce insulin, thereby limiting the use of insulin secretion as a determinant of BCM (4).

As an alternative to determine insulin secretion to quantify BCM, investigators evaluated a non-invasive positron emission tomography (PET) imaging technique to determine the BCM in rats with the use of ^11^C- or ^18^F-labeled dihydrotetrabenazine, which targets the vesicular monoamine transporter type 2 (VMAT2) in the pancreas (5-7). Although the VMAT2 has been used extensively for PET imaging of the brain in individuals suffering from Parkinson’s disease (8), its utilization for β cell imaging is still under investigation because the control of VMAT2 expression and function in these cells is not completely understood (4). The somatostatins (SST) and their receptors (SSTR) have not only been shown to be important for pancreatic development but are also implicated in diabetes mellitus and pancreatic cancer (9). Among the various SSTRs, SSTR1 and SSTR5 are considered to be biomarkers for the pancreatic β cells because they regulate insulin secretion and are found only in these cells (9, 10). Although several SST synthetic peptide analogs have been used to investigate the SSTRs (11), some non-peptide compounds have also been designed that show receptor specificity to the SSTRs, such as the SSTR1 (12). In an effort to develop an imaging compound for the measurement of BCM in the pancreas, a napthylalanine derivative, ^131^I-labeled N-{6-[(tert-butoxy)carbonylamino]-2,2,4-trimethylhexyl}-2-{[5-(1,1-dimethyl-1-stannaethyl)(3-pyridyl)]carbonylamino}-3-(2-napthyl)propanamide) ([^131^I]IPC-β-AL3), with a binding specificity for the SSTR1, was synthesized, radioiodinated with ^131^I, and studied for its biodistribution in normal and non-obese diabetic (NOD) mice by Amartey and colleagues (13, 14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IPC+beta+AL3+synthesis)]

The synthesis of IPC-β-AL3 was discussed in detail by Amartey et al. (13). Radioiodination with (^131^I)sodium iodide was performed with Iodogen as the oxidant in presence of a tin precursor as described elsewhere (13). The final product was purified on a Sep-Pak C_18_ cartridge, and purity of the labeled product ([^131^I]IPC-AL3) was established with high-performance liquid chromatography (HPLC). The radioiodinated product yield was reported to be 82 ± 8% (n = 7 reactions) when 100 μg of the precursor was used for the labeling reaction. The purity of [^131^I]IPC-AL3 was not reported. Specific activity of the labeled compound was reported to be 185 kBq/μg (5 μCi/μg). The stability of [^131^I]IPC-AL3 in human plasma, as determined with HPLC, was reported to be 93% after a 4-h exposure at ambient temperature (13). The radiochemical was reported to show 100% stability in phosphate-buffered saline under the same conditions.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IPC+beta+AL3+in+vitro)]

[^131^I]IPC-AL3 binding studies were performed using Chinese hamster ovary cells respectively transfected with SSTR1 and SST2 (14). The 50% inhibitory concentration values of [^131^I]IPC-AL3 for these receptors were reported to be 1.83 and 297 nM, respectively, indicating that the radiotracer had a >150-fold higher specificity for the SSTR1 than the SSTR2.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IPC+beta+AL3+rodentia)]

To determine the extent of [^131^I)IPC-AL3 uptake by the pancreas, Amartey et al. studied biodistribution of the radiochemical in normal CBA/J mice (13). The animals (n ≥ 4 mice/time point) were injected with the tracer and euthanized 15, 30, 60, and 120 min after treatment. The various organs and tissue of interest were harvested from the animals and counted for accumulated radioactivity (expressed as percent injected dose per gram tissue (% ID/g)). A rapid clearance of radioactivity from the blood was reported (1.0 ± 0.3% ID/g and 0.5 ± 0.2% ID/g at 15 min and 120 min, respectively). A high uptake of radioactivity was observed in the kidneys during the entire period of the study (23.0 ± 6.0% ID/g and 10.0 ± 2.0% ID/g at 15 min and 120 min, respectively). A similar trend was also noted in the intestines. The pancreas rapidly accumulated the label (18.0 ± 5.0% ID/g at 15 min), and a gradual loss of the tracer was observed subsequently (7.0 ± 3.0, 5.0 ± 0.6 and 3.9 ± 0.3% ID/g at 30, 60, and 120 min, respectively). Similar to the pancreas a high accumulation of radioactivity in the liver, spleen, and lungs was reported during the initial 15 min followed by a decline by 120 min.

Competition studies were also performed with another group of animals (n ≥ 4 mice/group) by injecting the radiolabel in presence of excess unlabeled IPC-β-AL3 (100 μg/mouse) (13). The control animals were treated with [^131^I]IPC-AL3 alone. The animals were euthanized 60 min after treatment and treated as described above. These animals showed a similar biodistribution of radioactivity as before, but a significant (P < 0.05) decrease in accumulation of radioactivity was noted in the spleen and pancreas. This indicated that the uptake of [^131^I]IPC-AL3 by the pancreas was probably mediated by the receptor.

In another study, the biodistribution of [^131^I]IPC-AL3 was compared in normal (CBA/J) and diabetic (NOD) mice of different age groups (5, 8, and 16 weeks, respectively; n ≥ 4 animals/group) as described by Amartey et al. (14). In general, the CBA/J mice had a higher uptake of radioactivity in all the organs, including the spleen and the pancreas (P < 0.05), compared with the NOD animals. The difference in uptake of radioactivity in the pancreas from the respective animal groups was confirmed with autoradiography.

From these studies the investigators concluded that, although [^131^I]IPC-AL3 had a high accumulation in the pancreas of normal and diabetic mice, [^131^I]IPC-AL3 may not be suitable for the imaging of β cells because this organ is in close proximity to the liver and the intestines, which also have a high accumulation of the label (14).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IPC+beta+AL3+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IPC+beta+AL3+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Concannon P., Rich S.S., Nepom G.T. (2009). Genetics of type 1A diabetes. N Engl J Med.
2 Krentz A.J., Bailey C.J. (2005). Oral antidiabetic agents: current role in type 2 diabetes mellitus. Drugs.
3 Ritzel R.A. (2009). Therapeutic approaches based on beta-cell mass preservation and/or regeneration. Front Biosci.
4 Harris P.E., Ferrara C., Barba P., Polito T., Freeby M., Maffei A. (2008). VMAT2 gene expression and function as it applies to imaging beta-cell mass. J Mol Med.
5 Simpson N.R., Souza F., Witkowski P., Maffei A., Raffo A., Herron A., Kilbourn M., Jurewicz A., Herold K., Liu E., Hardy M.A., Van Heertum R., Harris P.E. (2006). Visualizing pancreatic beta-cell mass with [11C]DTBZ. Nucl Med Biol.
6 Souza F., Simpson N., Raffo A., Saxena C., Maffei A., Hardy M., Kilbourn M., Goland R., Leibel R., Mann J.J., Van Heertum R., Harris P.E. (2006). Longitudinal noninvasive PET-based beta cell mass estimates in a spontaneous diabetes rat model. J Clin Invest.
7 Kung M.P., Hou C., Lieberman B.P., Oya S., Ponde D.E., Blankemeyer E., Skovronsky D., Kilbourn M.R., Kung H.F. (2008). In vivo imaging of beta-cell mass in rats using 18F-FP-(+)-DTBZ: a potential PET ligand for studying diabetes mellitus. J Nucl Med.
8 Collantes M., Prieto E., Penuelas I., Blesa J., Juri C., Marti-Climent J.M., Quincoces G., Arbizu J., Riverol M., Zubieta J.L., Rodriguez-Oroz M.C., Luquin M.R., Richter J.A., Obeso J.A. (2009). New MRI, 18F-DOPA and 11C-(+)-alpha-dihydrotetrabenazine templates for Macaca fascicularis neuroimaging: advantages to improve PET quantification. Neuroimage.
9 Ballian N., Brunicardi F.C., Wang X.P. (2006). Somatostatin and its receptors in the development of the endocrine pancreas. Pancreas.
10 Wang X.P., Norman M., Yang J., Magnusson J., Kreienkamp H.J., Richter D., DeMayo F.J., Brunicardi F.C. (2006). Alterations in glucose homeostasis in SSTR1 gene-ablated mice. Mol Cell Endocrinol.
11 Singh V., Brendel M.D., Zacharias S., Mergler S., Jahr H., Wiedenmann B., Bretzel R.G., Plockinger U., Strowski M.Z. (2007). Characterization of somatostatin receptor subtype-specific regulation of insulin and glucagon secretion: an in vitro study on isolated human pancreatic islets. J Clin Endocrinol Metab.
12 Wolkenberg S.E., Thut C.J. (2008). Recent progress in the discovery of selective, non-peptide ligands of somatostatin receptors. Curr Opin Drug Discov Devel.
13 Amartey J.K., Esguerra C., Al-Jammaz I., Parhar R.S., Al-Otaibi B. (2006). Synthesis and evaluation of radioiodinated substituted beta-naphthylalanine as a potential probe for pancreatic beta-cells imaging. Appl Radiat Isot.
14 Amartey J.K., Shi Y., Al-Jammaz I., Esguerra C., Al-Otaibi B., Al-Mohanna F. (2008). Radioiodinated naphthylalanine derivatives targeting pancreatic beta cells in normal and nonobese diabetic mice. Exp Diabetes Res.